# ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetracetic acid-Glu{PEG_4_-Glu[cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)}-{PEG_4_-Glu[cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)} (PEG_4_ = 15 amino-4,7,10,13-tetraoxapentadecanoic acid)

Chemical name: | ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetracetic acid-Glu{PEG_4_-Glu[cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)}-{PEG_4_-Glu[cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)} (PEG_4_ = 15 amino-4,7,10,13-tetraoxapentadecanoic acid) | [image]
Abbreviated name: | ^111^In(DOTA-2P4G-RGD_4_) | [image]
Synonym: | ^111^In-DOTA-E{PEG_4_-E[Gly_3_-c(RGDfK)]_2_}_2_ | [image]
Agent Category: | Peptides | [image]
Target: | Integrin alphavbeta3 (α_v_β_3_) | [image]
Target Category: | Receptors | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) or planar imaging | [image]
Source of signal / contrast: | ^111^In | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of ^111^In(DOTA-2P4G-RGD_4_) by Shi et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Integrin%20%u03B1v%u03B23%20and%20imaging)]

The ^111^In-labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetracetic acid (DOTA)-Glu{PEG_4_-Glu[cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)}-{PEG_4_-Glu[cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(Gly-Gly-Gly)-Arg-Gly-Asp-D-Phe)}, abbreviated as ^111^In(DOTA-2P4G-RGD_4_) or ^111^In-DOTA-E{PEG_4_-E[Gly_3_-c(RGDfK)]_2_}_2_, was synthesized by Shi et al. as an agent for molecular imaging of tumor angiogenesis by targeting integrin alphavbeta3 (α_v_β_3_) (1). Here, P = PEG_4_ = 15 amino-4,710,13-tetraoxapentadecanoic acid = a linker between two c(RGDfK) motifs; c(RGDfK) = cyclo(Lys-Arg-Gly-Asp-D-Phe); RGD_4_ = four motifs of c(RGDfK); E = Glu; and (G = G_3_ = Gly-Gly-Gly).

Integrin α_v_β_3_ is a receptor that is overexpressed on the activated endothelial cells of tumors (2). Because the integrin α_v_β_3_ binds with extracellular matrix proteins (e.g., vitronectin, fibronectin) through the exposed Arg-Gly-Asp tripeptide sequence, RGD-containing peptides have been intensively studied in the past decade as a vector for imaging α_v_β_3_ expression (3, 4). Although significant progress has been made, improving the binding affinity and pharmacokinetics of RGD peptides remains the major consideration in the design of agents, and various strategies have been developed for this improvement, such as the use of RGD multimers, the introduction of sugar amino acids or D-amino acids into the RGD peptides, and the conjugation of the RGD peptides with chelators or polyethylene glycol (PEG) chains (5, 6).

The concept of multimerization has been developed to address the question of multimeric binding by "poly-potent" ligands. Multimers are formed by bridging monomeric units through linker(s) (2, 7). The multimer effect has been demonstrated in different studies, showing that the binding affinity of RGD peptides increases in the order of monomer < dimer < tetramer < octamer. For example, the cyclo(-RGDfE-)-monomer, dimer, and tetramer containing heptaethylene glycol spacer units have been shown to exhibit α_v_β_3_-binding affinities that increase by a factor of ten with each duplication of binding units (8). The integrin affinity of the DOTA-RGD octamer has been shown to be three-fold higher than that of the DOTA-RGD tetramer (7).

Recently, investigators from Purdue University suggested a concept of "bivalency" for the α_v_β_3_-binding affinity of RGD-containing peptides (1, 6, 9). The main point of this concept is that the multimeric cyclic RGD peptides are likely bivalent rather than multivalent in binding to integrin α_v_β_3_, and enough distance between two RGD motifs is the key for bivalency (1, 5, 10). For example, the dimeric peptide E[c(RGDfK)]_2_ (RGD_2_) is monovalent, whereas the dimeric peptides PEG_4_-E[PEG_4_-c(RGDfK)]_2_ (3P-RGD_2_) and G_3_-E[G_3_-c(RGDfK)]_2_ (3G-RGD_2_) (G = G_3_ = Gly-Gly-Gly linker) are bivalent because of the increased distance between the two cyclic RGD motifs for simultaneous integrin α_v_β_3_ binding in the latter two peptides (5). The cyclic RGD tetramers, such as DOTA-RGD_4_ and DOTA-E{G_3_-E[G_3_-c(RGDfK)]_2_}_2_ (DOTA-6G-RGD_4_), are also likely bivalent in binding to integrin α_v_β_3_ even though they contain four identical RGD motifs (5, 10). Studies with three other tetramers (DOTA-2P-RGD_4_, DOTA-2P4G-RGD_4_, and DOTA-6P-RGD_4_) have further shown that the three tetramers are not tetravalent, although the tetramers exhibited a higher binding affinity to α_v_β_3_ than monomers and dimers, and the "locally enriched" RGD concentration has been considered to contribute to the higher binding affinity (1, 6). The linkers between RGD motifs may have a significant impact on the integrin α_v_β_3_-targeting capability, biodistribution, excretion kinetics, and metabolic stability of cyclic RGD peptides (1, 11, 12).

This chapter summarizes the data obtained with ^111^In(DOTA-2P4G-RGD_4_). Other chapters summarize the data obtained with ^111^In(DOTA-2P-RGD_4_) and ^111^In(DOTA-6P-RGD_4_), respectively.

### Related Resource Links:

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=integrin%20%CE%B1v%CE%B23) and protein (http://www.ncbi.nlm.nih.gov/protein?term=integrin%20%CE%B1v%CE%B23) sequences of integrin α_v_β_3_

Integrin α_v_β_3_-related imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=integrin+%CE%B1v%CE%B23+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Articles of integrin α_v_β_3_ (http://www.ncbi.nlm.nih.gov/omim?term=integrin%20%CE%B1v%CE%B23) in Online Mendelian Inheritance in Man

Integrin α_v_β_3_-related clinical trials (http://clinicaltrials.gov/ct2/results?term=integrin+%CE%B1v%CE%B23) in ClinicTrial.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%2021850213)]

The RGD-containing peptides were all custom-made, including P-RGD, P2G-RGD_2_, 3P-RGD_2_, and 3P-RGK_2_ (RGK = cyclo(Arg-Gly-Lys-D-Phe-Asp)). The tetramers were synthesized by the reaction of Boc-E(OSu)_2_ and their corresponding dimers (1). Conjugation of the RGD peptides with DOTA-OSu resulted in their corresponding conjugates (DOTA-P-RGD, DOTA-P-RGD_2_, DOTA-3P-RGD_2_, DOTA-2P-RGD_4_, DOTA-2P4G-RGD_4_, and DOTA-6P-RGD_4_, respectively). DOTA-6P-RGK_4_ was prepared using a procedure identical to that for DOTA-6P-RGD_4_. DOTA-6P-RGK_4_ has the identical amino acids, but its sequence is scrambled to demonstrate the RGD-specificity of DOTA-6P-RGD_4_. The identities for all RGD conjugates were confirmed, and their purities were all >95% before being used for ^111^In labeling and determination of their integrin α_v_β_3_ binding affinity. Table 1 lists the molecular weights and yields of each DOTA-conjugated peptide (1).

Table 1: The physicochemical characteristics of the RGD peptides.

Agents | DOTA-P-RGD | DOTA-P-RGD_2_ | DOTA-3P-RGD_2_* | DOTA-2P-RGD_4_ | DOTA-2P4G-RGD_4_ | DOTA-6P-RGD_4_ | DOTA-6P-RGK_4_
MW | 1,237.58 | 1,951.5 | 2,447.35 | 3,626.4 | 4,315.4 | 4,622.7 | 4,622.7
Yield | ~40% | ~41% | ~30% | ~56% | ~64% | ~43% | ~68%

*The data for DOTA-3P-RGD_2_ were obtained from Shi et al. (5).

All ^111^In-labeled peptides were prepared by reacting ^111^InCl_3_ with the respective DOTA conjugates in NH_4_OAc buffer (100 mM, pH = 5.5). Radiolabeling was completed by heating the reaction mixture at 100°C for ~15 min. After purification, the radiochemical purity was >95% and the specific activity was >40 mCi/μmol (1.48 GBq/µmol) for all ^111^In-labeled RGD peptides (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%2021850213)]

The integrin binding affinity and specificity of the RGD peptides were assessed in U87MG human glioma whole cells, with ^125^I-c(RGDyK) as the integrin-specific radioligand (1). The α_v_β_3_ binding affinity of the peptides followed the order of DOTA-6P-RGD_4_ ~ DOTA-2P4G-RGD_4_ ~ DOTA-2P-RGD_4_ > DOTA-P-RGD_2_ > DOTA-P-RGD > RGD (IC_50_ = 49.9 ± 5.5) (Table 1). The binding affinity of DOTA-3P-RGD_2_ was significantly higher than that of DOTA-P-RGD and DOTA-P-RGD_2_ (P < 0.01). However, the investigators found that the integrin α_v_β_3_ binding affinities of DOTA-2P-RGD_4_, DOTA-2P4G-RGD_4_, and DOTA-6P-RGD_4_ were only marginally higher than that of DOTA-3P-RGD_2_, suggesting that they might share the same bivalency in binding to the integrin α_v_β_3_.

Shi et al. also determined the water-octanol partition coefficients and stability of the ^111^In-labeled peptides (1). The log P values are listed in Table 2. The ^111^In-labeled peptides remained stable for >72 h after purification in the presence of 3 mM EDTA.

Table 2: The IC_50_ and log P values of the ^111^In-labeled cyclic RGD peptides.

Peptides | DOTA-P-RGD | DOTA-P-RGD_2_ | DOTA-3P-RGD_2_ | DOTA-2P-RGD_4_ | DOTA-2P4G-RGD_4_ | DOTA-6P-RGD_4_ | DOTA-6P-RGK_4_
IC_50_ (nM) | 44.3 | 5.0 | 1.5 | 0.5 | 0.2 | 0.3 | 437
Log P | -3.48 | -3.22 | -4.20 | -3.87 | -3.93 | -3.68 | -3.61

IC_50_: half-maximal inhibitory concentration.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%2021850213)]

Biodistribution, imaging, and metabolic studies were performed in athymic nude mice bearing U87MG human glioma xenografts in both left and right upper flanks (1).

For the biodistribution studies, each mouse was administered ~3 μCi (~0.111 MBq) of the agent via tail vein injection (1). Mice were then euthanized at 0.5, 1, 4, 24, and 72 h after injection (n = 5 mice/time point). The organ uptake was calculated as the percentage of injected dose per gram of organ mass (% ID/g). The tumor and intestinal uptakes of ^111^In(DOTA-2P-RGD_4_) were high and close to those of ^111^In(DOTA-6P-RGD_4_) over the 72-h period. ^111^In(DOTA-2P-RGD_4_) also had a rapid clearance from normal organs, such as the blood, kidneys, and liver. Therefore, the tumor/liver and tumor/kidney ratios of ^111^In(DOTA-2P-RGD_4_) were comparable to those obtained for ^111^In(DOTA-6P-RGD_4_) and ^111^In(DOTA-6G-RGD_4_.

Table 3: Selected biodistribution data of ^111^In(DOTA-2P-RGD_4_).

% ID/g | 0.5 h | 1 h | 24 h | 72 h
Blood | 0.84 ± 0.32 | 0.13 ± 0.00 | 0.02 ± 0.00 | 0.03 ± 0.01
Kidney | 10.72 ± 2.13 | 5.57 ± 0.63 | 1.98 ± 0.31 | 0.85 ± 0.09
Liver | 3.62 ± 0.85 | 2.36 ± 0.27 | 0.91 ± 0.08 | 0.25 ± 0.06
U87MG | 11.43 ± 2.92 | 10.18 ± 1.61 | 5.79 ± 0.67 | 2.66 ± 0.81
Tumor/Blood | 13.58 ± 3.47 | 80.74 ± 10.67 | 266.19 ± 59.02 | 93.96 ± 22.32
Tumor/Bone | 5.27 ± 1.35 | 5.80 ± 0.65 | 7.02 ± 1.39 | 6.76 ± 2.74
Tumor/Kidney | 1.07 ± 0.27 | 1.84 ± 0.26 | 2.96 ± 0.36 | 3.14 ± 0.84
Tumor/Liver | 3.15 ± 0.81 | 4.39 ± 1.13 | 6.46 ± 1.33 | 10.71 ± 1.45
Tumor/Lungs | 2.68 ± 0.69 | 4.38 ± 1.28 | 5.59 ± 0.63 | 8.73 ± 1.70
Tumor/Muscle | 6.99 ± 1.79 | 10.43 ± 1.75 | 24.04 ± 14.24 | 10.16 ± 2.72

No blocking experiment was performed with ^111^In(DOTA-2P4G-RGD_4_). The data obtained from blocking experiments with ^111^In(DOTA-6P-RGD_4_) are summarized in the chapter on ^111^In(DOTA-6P-RGD_4_) in MICAD (1).

The imaging studies were performed after tail vein administration of ~100 μCi (3.7 MBq) ^111^In(DOTA-2P4G-RGD_4_) (n = 3 mice) (1). The whole-body images were acquired at 0.5, 1, 4, 24, and 72 h after injection. The tumors were clearly visualized with excellent tumor/background contrast as early as 1 h after injection. A long tumor retention time was observed, which was consistent with the biodistribution results. The time to half-maximal radioactivity in tumors was >30 h for ^111^In(DOTA-2P-RGD_4_), ^111^In(DOTA-2P4G-RGD_4_), and ^111^In(DOTA-6P-RGD_4_) (1).

For the metabolism studies, each mouse was given ~100 μCi (3.7 MBq) ^111^In(DOTA-6P-RGD_4_) via tail vein injection (1). The urine samples were collected at 30 min and 120 min after injection, and the feces samples were collected at 120 min after injection. The percentage of radioactivity recovery was >95% (by γ-counting) for both urine and feces. There was very limited radioactivity accumulation in the liver and kidneys. There was little metabolism detected in the urine or feces samples over the 2-h study period for ^111^In(DOTA-2P4G-RGD_4_).

Shi et al. comparatively analyzed the biodistribution data for ^111^In(DOTA-2P-RGD_4_), ^111^In(DOTA-2P4G-RGD_4_), ^111^In(DOTA-6P-RGD_4_), ^111^In(DOTA-6G-RGD_4_), ^111^In(DOTA-3P-RGD_2_), ^111^In(DOTA-P-RGD_2_), and ^111^In(DOTA-P-RGD) (1). Over the first 24 h, the tumor uptake difference between the tetramers and dimers was not significant (P > 0.05). The tumor uptake at 72 h (% ID/g) followed the general order of ^111^In(DOTA-6P-RGD_4_) (3.04) > ^111^In(DOTA-2P-RGD_4_) (2.87) ~ ^111^In(DOTA-2P4G-RGD_4_) (2.66) > ^111^In(DOTA-3P-RGD_2_) (2.18), which was similar to the trend observed with integrin α_v_β_3_ binding affinity (IC_50_, nM) of DOTA-6P-RGD_4_ (0.3 ± 0.1) ~ DOTA-2P4G-RGD_4_ (0.2 ± 0.1) ~ DOTA-2P-RGD_4_ (0.5 ± 0.1) > DOTA-3P-RGD_2_ (1.5 ± 0.2). Among the ^111^In-labeled radiotracers, ^111^In(DOTA-6G-RGD_4_) had the highest uptake in the tumor and intestine at 72 h after injection. The half-life of ^111^In(DOTA-6G-RGD_4_) in the tumor was estimated to be 60 h. In contrast, ^111^In(DOTA-3P-RGD_2_) and ^111^In(DOTA-2P4G-RGD_4_) had low uptake in the intestine, kidneys, and liver over the 72-h period. As a result, ^111^In(DOTA-3P-RGD_2_) and ^111^In(DOTA-2P4G-RGD_4_) had tumor/kidney and tumor/liver ratios that were significantly better (P < 0.05) than those of ^111^In(DOTA-6G-RGD_4_) and ^111^In(DOTA-6P-RGD_4_) during that period of time. As expected, ^111^In(DOTA-P-RGD) had the lowest tumor uptake (3.7% ID/g and 0.7% ID/g at 0.5 h and 72 h after injection, respectively). ^111^In(DOTA-P-RGD_2_) had a relatively high tumor uptake (6.1 at 0.5 h after injection), but it had a significant washout from the tumor, with uptake values being 4.9, 4.8, 3.1, and 1.6% ID/g at 1, 4, 24, and 72 h after injection, respectively. The tumor uptake values follow the trend of ^111^In(DOTA-3P-RGD_2_) > ^111^In(DOTA-P-RGD_2_) > ^111^In(DOTA-P-RGD), which was consistent with the order of their α_v_β_3_ binding affinities (IC_50_ value): DOTA-3P-RGD_2_ < DOTA-P-RGD_2_ < DOTA-P-RGD.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed)]

No references are currently available.

## References

1 Shi J., et al. (2011). Evaluation of In-Labeled Cyclic RGD Peptides: Effects of Peptide and Linker Multiplicity on Their Tumor Uptake, Excretion Kinetics and Metabolic Stability. Theranostics.
2 Dijkgraaf I., Beer A.J., Wester H.J. (2009). Application of RGD-containing peptides as imaging probes for alphavbeta3 expression. Front Biosci.
3 Gaertner, F.C., M. Schwaiger, and A.J. Beer, Molecular imaging of avb3 expression in cancer patients. Q J Nucl Med Mol Imaging, 2010
4 Lu, X. and R.F. Wang, A Concise Review of Current Radiopharmaceuticals in Tumor Angiogenesis Imaging. Curr Pharm Des, 2012
5 Shi J., et al. (2011). Impact of bifunctional chelators on biological properties of 111In-labeled cyclic peptide RGD dimers. Amino Acids.
6 Liu S. (2009). Radiolabeled cyclic RGD peptides as integrin alpha(v)beta(3)-targeted radiotracers: maximizing binding affinity via bivalency. Bioconjug Chem.
7 Li Z.B., et al. (2007). (64)Cu-labeled tetrameric and octameric RGD peptides for small-animal PET of tumor alpha(v)beta(3) integrin expression. J Nucl Med.
8 Poethko T., et al. (2004). Chemoselective pre-conjugate radiohalogenation of unpretected mono- and multimeric peptides via oxime formation. Radiochim Acta.
9 Chakraborty S., et al. (2010). Evaluation of 111In-labeled cyclic RGD peptides: tetrameric not tetravalent. Bioconjug Chem.
10 Shi J., et al. (2009). Improving tumor uptake and pharmacokinetics of (64)Cu-labeled cyclic RGD peptide dimers with Gly(3) and PEG(4) linkers. Bioconjug Chem.
11 Liu Z., et al. (2009). (68)Ga-labeled cyclic RGD dimers with Gly3 and PEG4 linkers: promising agents for tumor integrin alphavbeta3 PET imaging. Eur J Nucl Med Mol Imaging.
12 Shi J., et al. (2008). Improving tumor uptake and excretion kinetics of 99mTc-labeled cyclic arginine-glycine-aspartic (RGD) dimers with triglycine linkers. J Med Chem.